# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-β max tris(acetic acid)-10-acetate mono(N-ethylmaleimide amide)-monomeric Z_HER2:477_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-β max tris(acetic acid)-10-acetate mono(N-ethylmaleimide amide)-monomeric Z_HER2:477_ | [image]
Abbreviated name: | ^64^Cu-DOTA-Z_HER2:477_ | [image]
Synonym: | | [image]
Agent Category: | Affibody, antibody | [image]
Target: | HER2 | [image]
Target Category: | Receptor | [image]
Method of detection: | PET | [image]
Source of signal / contrast: | ^64^Cu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of the agents by Cheng et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

The ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7-β max tris(acetic acid)-10-acetate mono(N-ethylmaleimide amide) (Mal-DOTA)-monomeric Z_HER2:477_ conjugate, abbreviated as ^64^Cu-DOTA-Z_HER2:477_, is an affibody derivative synthesized by Cheng et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that derive from the B-domain of staphylococcal surface protein A (2, 3). In the past several years, affibodies have drawn significant attention for developing imaging and therapeutic agents because of their unique features (3, 4). First, affibodies are small, with only 58 amino acid residues (~7 kDa) (3, 5). The small size allows affibodies to be generated with solid-phase peptide synthesis and to be cleared quickly from kidneys. Second, affibodies have a high binding affinity and specificity to their targets. Their binding affinity can be further improved by generating multimeric constructs through the solvent-exposed termini of affibody Z-domain. The anti-HER2 monomeric affibody Z_HER2:4_ is an example that has a binding affinity of ~50 nM, but its dimeric form, (Z_HER2:4_)_2_, exhibits an improved binding affinity up to ~3 nM (6). Third, affibodies lack cysteine residues and disulfide bridges in structure, and they fold rapidly. These features make it possible to chemically synthesize fully functional molecules and to introduce unique cysteine residues or chemical groups into affibodies for site-specific labeling. Several anti-HER2 affibody derivatives have been synthesized in this way. The imaging agent HPEM-His_6_-(Z_HER2:4_)_2_-Cys was generated by radiobrominating the dimeric (Z_HER2:4_)_2_ through the cysteine residues that were introduced to the C-terminus of (Z_HER2:4_)_2_ (7). Several affibody derivatives (e.g., ^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), and ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/)) were synthesized by coupling a chelating agent with a specifically protected site group of the Z_HER2:342_ peptide chain (3). Furthermore, these small affibody proteins can be selected and optimized with a strategy of sequence mutation and affinity maturation, and an example selected with this strategy is the anti-HER2 affibody Z_HER2:342_, which has an increased affinity from 50 nM to 22 pM (8).

The investigators at the Stanford University first tested the feasibility of the monomeric and dimeric forms of affibody Z_HER2:477_ for molecular imaging. Z_HER2:477_ is a commercially available anti-HER2 affibody. Both forms of the Z_HER2:477_ molecule were radiofluorinated with an ^18^F-labeled prosthetic group of 4-^18^F-fluorobenzaldehyde (^18^F-FBO-Z_HER2:477_ and ^18^F-FBO-(Z_HER2:477_)_2_, respectively) (9). The investigators have also coupled ^64^Cu to the affibody through DOTA, leading to the development of imaging agents of ^64^Cu-DOTA- Z_HER2:477_ and ^64^Cu-DOTA-(Z_HER2:477_)_2_ (1). Interestingly, these studies showed that smaller affibody constructs performed better in vivo in terms of tumor uptake and clearance. The investigators then generated a class of small proteins consisting of two α-helix bundles of the 3-helix affibody by deleting the helix 3 because the binding domain localizes in the α-helices 1 and 2 bundles (5). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles, with a disulfide bridge being formed between the two inserted homocysteines (10-12). The helix conformation of MUT-DS has been shown to be improved with the placement of a disulfide bridge. MUT-DS showed a binding affinity to HER2 in the low-nM range. The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for both imaging and therapy of HER2-expressing tumors.

This series of chapters summarizes the data obtained with the Z_HER2:477_ derivatives, and this chapter presents the data obtained with ^64^Cu-DOTA-Z_HER2:477_ (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-Benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-Benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/).

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The monomeric affibody Z_HER2:477_ with a purity of >95% is commercially available. The maleimide-functionalized chelator, Mal-DOTA, was synthesized with DOTA-mono-NHS-tris(tBu)ester, triethylamine, and N-(2-aminoethyl)maleimide-trifluoroacetic acid salt. The affibody Z_HER2:477_ was then modified at the cysteine residue of the C terminus with Mal-DOTA, which generated the conjugate DOTA-Z_HER2:477_ (1). The molecular weight of DOTA-Z_HER2:477_ was 7,277.50 Da with 25% recovery yield after purification. The conjugate was radiolabeled with ^64^Cu by incubation with ^64^CuCl_2_ for 1 h at 40°C. The product, ^64^Cu-DOTA-Z_HER2:477_, was purified on a PD-10 column and analyzed with radioanalytical high-performance liquid chromatography (HPLC).

The final product, ^64^Cu-DOTA-Z_HER2:477_, had a radiochemical purity of >95% and a specific activity of 29.1 MBq/nmol (786.5 µCi/nmol). HPLC analysis of the ^64^Cu-DOTA-Z_HER2:477_ showed a single peak with a retention time of 24.0 min. Octanol–water partition coefficient measurements showed a logP value of 0.018 ± 0.006, indicating intermediate hydrophilicity of the ^64^Cu-DOTA-Z_HER2:477_ (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Binding affinity with the extracellular domain of HER2 antigen was measured in vitro with surface plasmon resonance detection (1). Unlabeled DOTA-Z_HER2:477_ showed a binding affinity of 1.5 nM (100 pM for DOTA-(Z_HER2:477_)_2_) with association constants in the range of 10^5^ and dissociation constants in the range of 10−^4^–10−^5^, indicating that the on rate was very fast and the off rate was very slow. Binding affinity for ^64^Cu-DOTA-Z_HER2:477_ was not measured.

HER2 expression in SKOV3 human ovarian and MDA-MB-435 human breast cancer cells and tumor samples was verified with Western blot analysis (1). SKOV3 cells had high HER2 expression, whereas MDA-MB-435 cells expressed minimum HER2. The HER2 expression was 10–15-fold higher in SKOV3 tumors than in MDA-MB-435 tumors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Biodistribution studies were performed in nude mice bearing SKOV3 tumors (n = 3 mice/time point) (1). Mice were injected via the tail vein with 0.481–0.925 MBq (13–25 µCi) ^64^Cu-DOTA-Z_HER2:477_ and euthanized at 1, 4, and 20 h after injection, respectively. The radioactivity in ex vivo tissues was expressed as a percentage of the injected radioactive dose per gram of tissue (% ID/g). ^64^Cu-DOTA-Z_HER2:477_ exhibited rapid accumulation with moderate activity in the SKOV3 tumors at the early time point (3.86 ± 0.58% ID/g at 1 h), which increased to 6.12 ± 1.44% ID/g at 4 h and then dropped to 3.65 ± 0.69% ID/g over 20 h after injection. The tumor/blood ratios were 5.28 ± 0.91, 12.44 ± 3.39, and 5.12 ± 0.87, and the tumor/muscle ratios were 5.29 ± 1.61, 9.47 ± 2.46, and 7.23 ± 0.39 at 1, 4, and 20 h, respectively.

Comparison between ^64^Cu-DOTA-Z_HER2:477_ and its dimeric form ^64^Cu-DOTA-(Z_HER2:477_)_2_ showed that ^64^Cu-DOTA-Z_HER2:477_ had much higher tumor uptake than ^64^Cu-DOTA-(Z_HER2:477_)_2_ at all time points (P < 0.05). Both forms displayed rapid blood clearance, with 0.75 ± 0.22% ID/g and 2.27 ± 0.27% ID/g blood uptake at 1 h for ^64^Cu-DOTA-Z_HER2:477_ and ^64^Cu-DOTA-(Z_HER2:477_)_2_, respectively. Extremely high renal uptake and retention were found for both forms, but the renal uptake for monomeric ^64^Cu-DOTA-Z_HER2:477_ was 1–1.5-fold higher than that for ^64^Cu-DOTA-(Z_HER2:477_)_2_. The renal uptake values at 1, 4, and 20 h were 206.26 ± 22.36%, 237.51 ± 34.49%, and 129.69 ± 14.43% ID/g for ^64^Cu-DOTA-Z_HER2:477_ and 114.33 ± 11.22%, 75.21 ± 5.74%, and 37.95 ± 5.55% ID/g for ^64^Cu-DOTA-(Z_HER2:477_)_2_, respectively. Although relatively high liver uptake was observed for both agents, it was much lower than the renal uptake. Both forms exhibited relatively low uptake in all other normal organs.

PET imaging was performed in a mouse bearing SKOV3 and MDA-MB-435 tumors at 1, 4, and 20 h after tail vein injection of ^64^Cu-DOTA-Z_HER2:477_ (1). SKOV3 tumor was clearly visible with high tumor/background contrast at 1–20 h after injection. Only low uptake was observed in the MDA-MB-435 tumor, which makes it difficult to be visualized. Consistent with the biodistribution findings, high activity accumulation was observed in the kidneys.

To understand the relationship between ^64^Cu-DOTA-Z_HER2:477_ and Herceptin (trastuzamab), mice bearing SKOV3 tumors (n = 6 mice) were pretreated with 300 µg Herceptin or phosphate-buffered saline via tail vein injection. At 48 h after pretreatment, the mice were injected with ^64^Cu-DOTA-Z_HER2:477_ (2.59–3.14 MBq (70–85 μCi)) and imaged at 1, 3.5, and 24 h. Pretreatment with Herceptin reduced the uptake of ^64^Cu-DOTA-Z_HER2:477_ in SKOV3 tumors, indicating that Herceptin blocks the binding of ^64^Cu-DOTA-Z_HER2:477_. Blocking studies were not performed for the dimeric form.

In conclusion, the ^64^Cu-labeled dimer and monomer exhibited rapid tumor accumulation and blood clearance, which are favorable for imaging (1). Although the dimeric form exhibited higher HER2-binding affinity than did the monomeric form, the dimeric form showed much lower SKOV3 tumor accumulation and tumor/normal organ ratios than that of the monomeric form. The blocking results with Herceptin and affibody molecules are controversial in the literature, and the use of different affibody clones may be partially responsible for the controversy (4, 6). Very high kidney uptake and retention for both agents are likely to be a concern for their clinical use, and further optimization is necessary (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Tolmachev V., Orlova A., Nilsson F.Y., Feldwisch J., Wennborg A., Abrahmsen L. (2007). Affibody molecules: potential for in vivo imaging of molecular targets for cancer therapy. Expert Opin Biol Ther.
5 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
6 Steffen A.C., Wikman M., Tolmachev V., Adams G.P., Nilsson F.Y., Stahl S., Carlsson J. (2005). In vitro characterization of a bivalent anti-HER-2 affibody with potential for radionuclide-based diagnostics. Cancer Biother Radiopharm.
7 Mume E., Orlova A., Larsson B., Nilsson A.S., Nilsson F.Y., Sjoberg S., Tolmachev V. (2005). Evaluation of ((4-hydroxyphenyl)ethyl)maleimide for site-specific radiobromination of anti-HER2 affibody. Bioconjug Chem.
8 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
9 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
10 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
11 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
12 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.